# ^68^Ga-1,4,7,10-Tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid-Gly-Gly-Gly-Gly-Lys-Gly-Gly-Gly-Gly

Chemical name: | ^68^Ga-1,4,7,10-Tetraazacyclododecane-N, N',N'',N'''-tetraacetic acid-Gly-Gly-Gly-Gly-Lys-Gly-Gly-Gly-Gly
Abbreviated name: | ^68^Ga-DOTA-VAP-P1
Synonym:
Agent Category: | Peptide
Target: | Cell adhesion protein 1/semicarbazide-sensitive monoamine oxidase (VAP-1/SSAO)
Target Category: | SSAO inhibition
Method of detection: | PET
Source of signal: | ^68^Ga
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=54648638), nucleotide (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=nuccore&id=46249772) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?db=gene&cmd=Retrieve&dopt=full_report&list_uids=7412) for more information about VAP-1.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VAP-1)]

Endothelial cells are important cells in inflammatory responses (1, 2). Bacterial lipopolysaccharide (LPS), virus, inflammation, and tissue injury increase tumor necrosis factor α (TNFα), interleukin-1 (IL-1), and other cytokine and chemokine secretion. Leukocyte emigration from blood is dependent on their ability to roll along endothelial cell surfaces and subsequently adhere to endothelial cell surfaces. Inflammatory mediators and cytokines induce chemokine secretion from endothelial cells and other vascular cells and increase their expression of cell-surface adhesion molecules, such as intracellular adhesion molecule-1 (ICAM-1), vascular cell adhesion molecule-1 (VCAM-1), integrins, and selectins. Chemokines are chemotactic toward leukocytes and toward sites of inflammation and tissue injury. The movements of leukocytes through endothelial junctions into the extravascular space are highly orchestrated through various interactions with different adhesion molecules on endothelial cells (3).

Cell adhesion protein 1 (VAP-1) is not usually expressed on the cell surface of resting endothelial cells (4, 5). VAP-1 is a dual-function protein with adhesion properties and semicarbazide-sensitive monoamine oxidase (SSAO) activity. VAP-1 binds to its counterpart receptors on the cell surface of leukocytes. Inflammation increases expression of VAP-1 and other cell adhesion molecules on the vascular endothelial cells (4, 5), which leads to leukocyte adhesion to the activated endothelium and transmigration (6). Using a molecular model of VAP-1, a linear peptide of nine amino acids (Gly-Gly-Gly-Gly-Lys-Gly-Gly-Gly-Gly) (VAP-P1) was found to inhibit the SSAO activity of recombinant VAP-1 and block leukocyte–endothelium interactions (7). ^68^Ga (half-life = 68 min, 89% β^+^ decay) is an attractive radionuclide for labeling VAP-P1 and is readily available from a commercial ^68^Ge/^68^Ga generator (8). Cells retain ^68^Ga well, providing a good signal/background ratio. For evaluation as a positron emission tomography (PET) imaging agent for inflammatory and infectious processes in healing bones, ^68^Ga has been attached to VAP-P1 via 1,4,7,10-tetraazacyclododecane-N,N',N'',N'''-tetraacetic acid (DOTA) to form ^68^Ga-DOTA-VAP-P1 (9).

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VAP-P1+and+synthesis)]

Commercially available DOTA-tris(tert-butylester) (Macrocyclics, Dallas, TX) was used to conjugate the N-terminal amino acid to form DOTA-VAP-P1 after standard solid-phase peptide synthesis of VAP-P1 (9). DOTA-VAP-P1 (DOTA/VAP-P1 ratio, ~1) was purified with high-performance liquid chromatography. ^68^GaCl_3_ was conjugated to DOTA-VAP-P1 (30 nmol) by incubation at 100°C for 20 min. ^68^Ga-DOTA-VAP-P1 had >95% radiochemical purity with a specific activity of 94 ± 29 MBq/nmol (2.54 ± 0.78 mCi/nmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VAP-P1+and+in+vitro)]

Yegutkin et al. (7) showed that VAP-P1 inhibited the SSAO activity of recombinant VAP-1 with an IC_50_ value of 534 ± 28 μM (n = 12), whereas no inhibition was observed with other amine oxidases tested, such as diamine oxidase or mitochondrial monoamine oxidase. VAP-P1 also inhibited lymphocyte interactions with rabbit endothelial cells in vitro by 30–40% at 500 μM via inhibition of the SSAO activity of the rabbit endothelial cells.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VAP-P1+and+rodentia)]

Lankinen et al. (9) performed PET imaging with ^68^Ga-DOTA-VAP-P1 in 34 rats with diffuse Staphylococcus aureus tibial osteomyelitis (infectious bone healing) and 34 rats with healing cortical bone defects (as control with inflammatory/normal healing) using at 0.5, 1, 1.5, 7, 14, and 28 days after surgery. The mean standard uptake values (SUVs) of the infected bone area in the osteomyelitic animals were 1.17 ± 0.74 and 2.28 ± 0.93 at 1 day and 7 days after surgery, respectively. The mean SUVs of the operated bone area in control animals were 1.37 ± 0.70 and 1.08 ± 0.54 at 1 day and 7 days after surgery, respectively. The osteomyelitic and control animals showed a similar uptake of the ^68^Ga-DOTA-VAP-P1 at 1 day, whereas a significant difference was observed at 7 days (P < 0.0001). In osteomyelitic animals, the mean SUV ratio of the osteomyelitic tibia (1.50 ± 0.16) at 1 day and (1.87 ± 0.41) 7 days after surgery was higher than that of the contralateral intact tibia (P = 0.0016). In the control animals with healing bone defects, the corresponding mean SUV ratios at 1 day and 7 days after surgery were 1.48 ± 0.18 and 1.09 ± 0.08, respectively, which represents a significant decrease in the uptake between the two time points (P = 0.0008). The SUV ratios of osteomyelitic animals imaged 7 days after surgery differed significantly (P < 0.0001) from those of the corresponding control animals with healing bone defects. In contrast, the difference in SUV ratios between osteomyelitic and control animals imaged 1 day after surgery was not statistically significant. Microbiological and histopathological analyses showed corresponding inflammatory cell grade and VAP-1 expression in PET imaging with ^68^Ga-DOTA-VAP-P1. PET imaging showed an uptake of ^68^Ga-DOTA-VAP-P1 in both the osteomyelitic bones and the healing cortical bone defects during the first day after surgery. In contrast, PET imaging showed uptake only in the osteomyelitic tibias after the first day.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VAP-P1+and+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VAP-P1+and+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=VAP-P1+and+human)]

No publication is currently available.

## References

1 Cybulsky M.I., Gimbrone M.A. (1991). Endothelial expression of a mononuclear leukocyte adhesion molecule during atherogenesis. Science.
2 Lowe J.B. (2002). Glycosylation in the control of selectin counter-receptor structure and function. Immunol Rev.
3 Vanderslice P., Woodside D.G. (2006). Integrin antagonists as therapeutics for inflammatory diseases. Expert Opin Investig Drugs.
4 Jalkanen S., Salmi M. (2008). VAP-1 and CD73, endothelial cell surface enzymes in leukocyte extravasation. Arterioscler Thromb Vasc Biol.
5 Salmi M., Jalkanen S. (2001). VAP-1: an adhesin and an enzyme. Trends Immunol.
6 Jalkanen S., Karikoski M., Mercier N., Koskinen K., Henttinen T., Elima K., Salmivirta K., Salmi M. (2007). The oxidase activity of vascular adhesion protein-1 (VAP-1) induces endothelial E- and P-selectins and leukocyte binding. Blood.
7 Yegutkin G.G., Salminen T., Koskinen K., Kurtis C., McPherson M.J., Jalkanen S., Salmi M. (2004). A peptide inhibitor of vascular adhesion protein-1 (VAP-1) blocks leukocyte-endothelium interactions under shear stress. Eur J Immunol.
8 Maecke H.R., Hofmann M., Haberkorn U. (2005). (68)Ga-labeled peptides in tumor imaging. J Nucl Med.
9 Lankinen P., Makinen T.J., Poyhonen T.A., Virsu P., Salomaki S., Hakanen A.J., Jalkanen S., Aro H.T., Roivainen A. (2008). (68)Ga-DOTAVAP-P1 PET imaging capable of demonstrating the phase of inflammation in healing bones and the progress of infection in osteomyelitic bones. Eur J Nucl Med Mol Imaging.